# 2β-Carbomethoxy-3β-(4-chlorophenyl)-8-(2-[^18^F]fluoroethyl)nortropane

Chemical name: | 2β-Carbomethoxy-3β-(4-chlorophenyl)-8-(2-[^18^F]fluoroethyl)nortropane
Abbreviated name: | [^18^F]FECNT
Synonym:
Agent Category: | Compound
Target: | Dopamine transporter
Target Category: | Binding to dopamine transporter
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FECNT%5BAll%20Fields%5D)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion. Parkinson’s disease (PD) is associated with a loss of dopamine-containing neurons in the striatum, resulting in a loss of dopamine transporter (DAT) protein in the presynaptic nerve terminals (1, 2). DAT is important to the regulation of synaptic concentration of dopamine. However, reduction of DAT density is not necessarily a measure of the clinical severity of motor dysfunction in PD patients (3). Several cocaine analogs were developed for the evaluation of DAT density in striatal neurons of PD patients (4). Radiolabeled 2β-carboxymethoxy-3β-(4-iodophenyl)tropane (β-CIT) and N-(3-fluoropropyl)-2β-carbomethoxy-3β-(4-iodophenyl)nortropane (FP-CIT) have been used for brain imaging (5-8). [^123^I]β-CIT was studied in humans in single photon emission computed tomography (SPECT), which showed slow tracer uptake kinetics (9, 10). ^123^I tracer allows delayed scanning. [^18^F]FP-CIT has been evaluated in humans (6). A switch was made to ^18^F to gain better resolution and quantitation. However, the radiochemical yields were reported to be 1-4% (6, 8). This led to the development of 2β-carbomethoxy-3β-(4-chlorophenyl)-8-(2-[^18^F]fluoroethyl)nortropane ([^18^F]FECNT) for positron emission tomography (PET) brain imaging in PD patients.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FECNT%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D)]

[^18^F]FECNT was synthesized by preparation of 1-[^18^F]fluoro-2-tosyloxyethane using the standard potassium [^18^F]fluoride Kryptofix complex, followed by alkylation of 2β-carbomethoxy-3β-(4-chlorophenyl)nortropane (11). This method provided a radiochemical yield of 21% (decay corrected to the end of bombardment) in 122 min, including high-performance liquid chromatography (HPLC) purification and a radiochemical purity of >99%, with a specific activity of 74 GBq/μmol (2 Ci/μmol).

In another synthesis, 2-[^18^F]fluoro-1-(4-bromobenzenesulfonate)-ethanol was prepared by a nucleophilic fluorination of 1,2-ethanediol bis-(4-bromobenzenesulfonate) with potassium [^18^F]fluoride Kryptofix complex (12). 2-[^18^F]Fluoro-1-(4-bromobenzenesulfonate)-ethanol was used to alkylate 2β-carbomethoxy-3β-(4-chlorophenyl)nortropane to form [^18^F]FECNT. The radiochemical yield of [^18^F]FECNT was 16.5 ± 5.3%, and its radiochemical purity was 99.8%. The average specific activity was 38 ± 45 GBq/μmol (1.03 ± 1.22 Ci/μmol) at the end of bombardment. This method was later automated by Voll et al. (13) to reliably produce [^18^F]FECNT in a 16% decay-corrected yield in a total time of 150 min. The specific activity of [^18^F]FECNT was 74-92 GBq/μmol (2-2.5 Ci/μmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FECNT%5BAll%20Fields%5D%20AND%20%28%22in%20vitro%22%5BMeSH%20Terms%5D%20OR%20in%20vitro%5BText%20Word%5D%29)]

FECNT was reported to bind selectively to human dopaminergic transporter (11). Binding affinities (K_i_, nM) of FECNT for human DAT, serotonin transporter (SERT), and norepinephrine transporter (NET) were 1.53, 39.1, and 240, respectively. Selective binding to the DAT versus SERT and NET was also observed in rat brain homogenates with FECNT.

In vitro autoradiograms showed that the binding of [^18^F]FECNT was localized to the caudate nucleus and putamen of cortical sections of monkey brain. The DAT inhibitors GBR 12909 (100 nM) and CIT (100 nM) were able to block the [^18^F]FECNT binding in the caudate and putamen by 50% and 85%, respectively. On the other hand, the serotonin reuptake inhibitor paroxetine (100 nM) showed little inhibition of [^18^F]FECNT striatal binding.

## Animal Studies

### Rodents

[PubMed] (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FECNT%20and%20rodentia)

Blocking studies of [^18^F]FECNT binding to DAT by monoamine transporter inhibitors (5 mg/kg) were performed in rats (11). Brain uptake was the highest in the striatum (2.24% injected dose (ID)/g), followed by prefrontal cortex (1.17%), hypothalamus (1.00%), cortex (0.57%), and cerebellum (0.28%) at 60 min after injection of 2.2 MBq (0.06 mCI) of [^18^F]FECNT. The uptake of [^18^F]FECNT in the striatum was blocked only by the DAT inhibitor GBR 12909. The SERT inhibitor paroxetine and NET inhibitor reboxetine exhibited no effect on the striatal uptake of [^18^F]FECNT.

Honer et al. (14) performed [^18^F]FECNT PET studies in mice showing a good visualization of the striatum from 1 to 30 min with low accumulation in the cerebellum. However, there was a fast washout from the striatum and the striatal radioactivity was similar to that of the cerebellum by 50 min. 1-methyl-4-phenyl-1,2,3,6-tetrahydropyridine (MPTP) (4X20 mg/kg) inhibited the striatal accumulation by 57% (P = 0.008) as compared with control mice.

Zoghbi et al. (15) showed that [^18^F]FECNT accumulated ~7-fold higher in the striatum than in the cortex and cerebellum at 60 min after the injection of 2 rats. The fraction of intact [^18^F]FECNT in striatum was 90 and 71% at 60 and 120 min, respectively, whereas 59 and 13% in the cerebellum and 13 and 10% in the plasma. A radiometabolite was distributed at equal concentrations in all brain regions. The LC-MS analyses identified N-dealkylated FECNT as a major metabolite in the rat brain. The radiometabolite likely was [^18^F]fluoroacetaldehyde, the product expected from the N-dealkylation of 18F-FECNT, or its oxidation product, [^18^F]fluoroacetic acid. [^18^F]FECNT was shown to be stable in both rat whole blood and brain homogenates at 37°C up to 4 h. Zoghbi et al. (15) suggested that the radiometabolite was formed by P-450 oxidative metabolism in the liver and then accumulated uniformly in the brain.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FECNT%20and%20%28dog%20or%20rabbit%20or%20sheep%20or%20pig%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%20and%20FECNT%29%20and%20monkey)]

[^18^F]FECNT PET studies were performed in rhesus monkeys (8). [^18^F]FECNT entered the brain rapidly. There was a high uptake in the caudate and putamen, resulting in caudate- and putamen-to-cerebellum ratios of 10.5 at 60 min. After pretreatment with CIT (0.9 μmol/kg), radioactivity in the striatum was markedly reduced, thus indicating specific [^18^F]FECNT binding to the DAT. The fraction of unchanged [^18^F]FECNT in monkey plasma determined by HPLC was 91% at 2 min, 33% at 15 min, and 6% at 120 min.

Cocaine at doses that maintained maximum response rates was shown to decrease DAT occupancy by 53-87%, as determined by displacement of [^18^F]FECNT in monkey brains (16). Similar results were observed with cocaine and cocaine analogs in other studies of monkeys (17, 18). Isoflurane, an anesthetic, was shown to decrease [^18^F]FECNT binding potential in rhesus monkeys by 63% with no significant change in total DAT protein in the striatum (19). Control monkeys were administered 1% isoflurane, and experimental monkeys were administered 2% isoflurane.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FECNT%20and%20human)]

Human dosimetry of [^18^F]FECNT was determined from biodistribution and PET imaging data from rats and monkeys after intravenous injection of [^18^F]FECNT (20). The organ that received the highest dose was the basal ganglia (0.105 mGy/MBq or 387 mrad/mCi), followed by the heart (0.0417 mGy/MBq or 154 mrad/mCi) and the intestine (0.0175 mGy/MBq or 65 mrad/mCi). The effective dose equivalent was 0.018 mSv/MBq (67 mrem/mCi). In a later study, Tipre et al. (21) reported the effective dose equivalent to be 0.0273-0.0276 mSv/MBq (98-102 mrem/mCi) in rhesus monkeys after injection of 185 MBq (5 mCi) of [^18^F]FECNT.

[^18^F]FECNT PET was first studied in 6 normal subjects and 5 PD patients (12). A higher uptake into striatal regions was observed in the normal brain than the PD brain. The caudate and putamen reached maximum radioactivity at 90 min with healthy subjects, with average caudate- and putamen-to-cerebellum ratios of 9.0 ± 1.2 and 7.8 ± 0.7, respectively. A reduction in basal ganglia uptake of >60% was observed in the PD patients. Only 40% of [^18^F]FECNT remained in the plasma at 20 min after injection. HPLC plasma analysis indicated the presence of only one major polar metabolite. An [^18^F]FECNT PET scan is a useful tool to reveal the state of dopamine occupancy of DAT in the brain.

Zoghbi et al. (15) performed comparative [^18^F]FECNT PET studies in 3 monkeys and 2 humans. The plasma free fractions of [^18^F]FECNT were 9.4% ± 2.7% (n = 6) in monkeys and 4.7% ± 1.3% (n = 4) in humans. At ~6 min after the administration of [^18^F]FECNT, monkey plasma was composed of 50% radiometabolite and 50% parent [^18^F]FECNT. The 50% radiometabolite/ 50% parent composition occurred at 18 and 27 min after injection in humans. The distribution volume in the cerebellum increased up to 1.7-fold in humans between 60 and 300 min after injection and 2.0-fold in monkeys between 60 and 240 min after injection. Plasma [^18^F]FECNT was used as the input function for compartmental nonlinear least squares analysis. The increases suggest an entry of radiometabolite into the cerebellum. On the other hand, the distribution volume in the striatum did not increase during the same time points. Zoghbi et al. (15) suggested that analysis using the cerebellum as the reference region would produce more variations than a measured arterial input function.

## Supplemental Information

[Disclaimers]

Toxicology

Animal Dosimetry

Human Dosimetry

## NIH Support

Intramural research program, R01 GM63824, RR-00165,

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Ravina B., Eidelberg D., Ahlskog J.E., Albin R.L., Brooks D.J., Carbon M., Dhawan V., Feigin A., Fahn S., Guttman M., Gwinn-Hardy K., McFarland H., Innis R., Katz R.G., Kieburtz K., Kish S.J., Lange N., Langston J.W., Marek K., Morin L., Moy C., Murphy D., Oertel W.H., Oliver G., Palesch Y., Powers W., Seibyl J., Sethi K.D., Shults C.W., Sheehy P., Stoessl A.J., Holloway R. (2005). The role of radiotracer imaging in Parkinson disease. Neurology.
4 Scheffel U., Dannals R.F., Wong D.F., Yokoi F., Carroll F.I., Kuhar M.J. (1992). Dopamine transporter imaging with novel, selective cocaine analogs. Neuroreport.
5 Abi-Dargham A., Gandelman M.S., DeErausquin G.A., Zea-Ponce Y., Zoghbi S.S., Baldwin R.M., Laruelle M., Charney D.S., Hoffer P.B., Neumeyer J.L., Innis R.B. (1996). SPECT imaging of dopamine transporters in human brain with iodine-123-fluoroalkyl analogs of beta-CIT. J Nucl Med.
6 Chaly T., Dhawan V., Kazumata K., Antonini A., Margouleff C., Dahl J.R., Belakhlef A., Margouleff D., Yee A., Wang S., Tamagnan G., Neumeyer J.L., Eidelberg D. (1996). Radiosynthesis of [18F] N-3-fluoropropyl-2-beta-carbomethoxy-3-beta-(4-iodophenyl) nortropane and the first human study with positron emission tomography. Nucl Med Biol.
7 Kazumata K., Dhawan V., Chaly T., Antonini A., Margouleff C., Belakhlef A., Neumeyer J., Eidelberg D. (1998). Dopamine transporter imaging with fluorine-18-FPCIT and PET. J Nucl Med.
8 Lundkvist C., Halldin C., Ginovart N., Swahn C.G., Farde L. (1997). [18F] beta-CIT-FP is superior to [11C] beta-CIT-FP for quantitation of the dopamine transporter. Nucl Med Biol.
9 Ishikawa T., Dhawan V., Kazumata K., Chaly T., Mandel F., Neumeyer J., Margouleff C., Babchyck B., Zanzi I., Eidelberg D. (1996). Comparative nigrostriatal dopaminergic imaging with iodine-123-beta CIT-FP/SPECT and fluorine-18-FDOPA/PET. J Nucl Med.
10 Laruelle M., Wallace E., Seibyl J.P., Baldwin R.M., Zea-Ponce Y., Zoghbi S.S., Neumeyer J.L., Charney D.S., Hoffer P.B., Innis R.B. (1994). Graphical, kinetic, and equilibrium analyses of in vivo [123I] beta-CIT binding to dopamine transporters in healthy human subjects. J Cereb Blood Flow Metab.
11 Goodman M.M., Kilts C.D., Keil R., Shi B., Martarello L., Xing D., Votaw J., Ely T.D., Lambert P., Owens M.J., Camp V.M., Malveaux E., Hoffman J.M. (2000). 18F-labeled FECNT: a selective radioligand for PET imaging of brain dopamine transporters. Nucl Med Biol.
12 Davis M.R., Votaw J.R., Bremner J.D., Byas-Smith M.G., Faber T.L., Voll R.J., Hoffman J.M., Grafton S.T., Kilts C.D., Goodman M.M. (2003). Initial human PET imaging studies with the dopamine transporter ligand 18F-FECNT. J Nucl Med.
13 Voll R.J., McConathy J., Waldrep M.S., Crowe R.J., Goodman M.M. (2005). Semi-automated preparation of the dopamine transporter ligand [(18)F]FECNT for human PET imaging studies. Appl Radiat Isot.
14 Honer M., Hengerer B., Blagoev M., Hintermann S., Waldmeier P., Schubiger P.A., Ametamey S.M. (2006). Comparison of [18F]FDOPA, [18F]FMT and [18F]FECNT for imaging dopaminergic neurotransmission in mice. Nucl Med Biol.
15 Zoghbi S.S., Shetty H.U., Ichise M., Fujita M., Imaizumi M., Liow J.S., Shah J., Musachio J.L., Pike V.W., Innis R.B. (2006). PET imaging of the dopamine transporter with 18F-FECNT: a polar radiometabolite confounds brain radioligand measurements. J Nucl Med.
16 Votaw J.R., Howell L.L., Martarello L., Hoffman J.M., Kilts C.D., Lindsey K.P., Goodman M.M. (2002). Measurement of dopamine transporter occupancy for multiple injections of cocaine using a single injection of [F-18]FECNT. Synapse.
17 Wilcox K.M., Kimmel H.L., Lindsey K.P., Votaw J.R., Goodman M.M., Howell L.L. (2005). In vivo comparison of the reinforcing and dopamine transporter effects of local anesthetics in rhesus monkeys. Synapse.
18 Wilcox K.M., Lindsey K.P., Votaw J.R., Goodman M.M., Martarello L., Carroll F.I., Howell L.L. (2002). Self-administration of cocaine and the cocaine analog RTI-113: relationship to dopamine transporter occupancy determined by PET neuroimaging in rhesus monkeys. Synapse.
19 Votaw J., Byas-Smith M., Hua J., Voll R., Martarello L., Levey A.I., Bowman F.D., Goodman M. (2003). Interaction of isoflurane with the dopamine transporter. Anesthesiology.
20 Deterding T.A., Votaw J.R., Wang C.K., Eshima D., Eshima L., Keil R., Malveaux E., Kilts C.D., Goodman M.M., Hoffman J.M. (2001). Biodistribution and radiation dosimetry of the dopamine transporter ligand. J Nucl Med.
21 Tipre D.N., Fujita M., Chin F.T., Seneca N., Vines D., Liow J.S., Pike V.W., Innis R.B. (2004). Whole-body biodistribution and radiation dosimetry estimates for the PET dopamine transporter probe 18F-FECNT in non-human primates. Nucl Med Commun.